# ^111^In-Labeled CHX-A”-DTPA conjugated monoclonal antibody (mAb) 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)

Chemical name: | ^111^In-Labeled CHX-A”-DTPA conjugated monoclonal antibody (mAb) 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Abbreviated name: | [^111^In]-mAb806
Synonym: | [^111^In]-CHX-A”-DTPA-mAb806
Agent Category: | Antibody
Target: | Epidermal growth factor receptor deletion variant de2-7 (EGFRvIII)
Target Category: | Receptor
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure information available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ch806&cmd=DetailsSearch)]

The biological characteristics, activating ligands, and functioning of the different members of the transmembrane epidermal growth factor receptor (EGFR) family are described elsewhere (1-3). These receptors are known to regulate the growth, survival, differentiation, and migration of cells through the activation of an associated intracellular tyrosine kinase (TK) signaling pathway, and they are overexpressed in many malignant epithelial tumors (1, 2). In addition, overexpression of the EGFR usually indicates a poor clinical prognosis for the patient (4). Overexpression of the EGFR in the tumors has been attributed to gene amplification, and this phenomenon is believed to introduce mutations in the receptor (2, 4). The most common mutation observed in the EGFR receptor is the deletion of a segment of the EGFR extracellular domain, including the ligand-binding region, which results in the generation of an EGFR variant known as the de2-7 EGFR or EGFRvIII (2, 4). The generation, structure, functions, and role of EGFRvIII in tumor malignancy have been reviewed by Gan et al. (5). Although EGFRvIII is nonresponsive to the ligand, it is constitutively active with a constantly operating downstream TK signal transduction pathway that appears to promote the development of a neoplastic phenotype, particularly for glioblastoma and to some extent for other cancers such as those of the prostate and the breast (2, 6).

Because the EGFR promotes and helps maintain the cancerous state of cells, several antibodies that inhibit the receptor activity and small molecules that block the downstream TK signaling pathway have been developed and have been approved by the United States Food and Drug Administration (FDA) for the treatment of certain cancers (2). The antibodies are directed toward the extracellular domain of the receptor, block ligand binding, and inhibit activation of the TK signal transduction pathway, which ultimately results in downregulation of the EGFR on the cell surface. However, because the EGFRvIII lacks the ligand-binding region on the extracellular domain, these antibodies cannot obstruct the constitutive mutant receptor activity (2). As a consequence, the monoclonal antibody (mAb) 806, which specifically targets the EGFRvIII, was generated and characterized in preclinical studies (7, 8). Subsequently, a chimeric form of the mAb (chAb), designated as ch806, was developed and evaluated in a phase I clinical trial with patients having cancerous tumors overexpressing the EGFRvIII (4). Results obtained from this trial indicated that ch806 could be a good biotherapeutic agent for the treatment of cancers expressing the ch806 antigen (4). In addition, several other clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) approved by the FDA are in progress to evaluate the targeting of EGFRvIII as a treatment against various cancers.

The internalization, intracellular trafficking, and biodistribution (in nude mice bearing xenograft human epidermoid carcinoma cell tumors) of mAb806 labeled with ^111^In ([^111^In]-mAb806) and ^125^I ([^125^I]-mAb806) have been investigated by Perera et al. (8). The characterization and biodistribution (in nude mice bearing xenograft human glioblastoma cell tumors) of ch806 labeled with ^125^I and ^111^In, respectively, are described in separate chapters in MICAD (www.micad.nih.gov) (9, 10). Another chapter describes the use of ^124^I-labeled ch806 for the detection of EGFRvIII-expressing xenograft human glioblastoma tumors in nude mice with an immuno–positron emission tomography (PET) technique (11). This chapter describes the studies performed with [^111^In]-mAb806. Studies performed with [^125^I]-mAb806 are described in a separate chapter in MICAD (12).

### Other sources of information

Human EGFR Gene (http://www.ncbi.nlm.nih.gov/gene/1956) (Gene ID: 1956)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim/131550) (Online Mendelian Inheritance in Man)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?what=graphic&jpg=on&pathway_id=200131&source=NATURE&output-format=graphic&ppage=1&genes_a=1956) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Related chapters (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20synthesis&cmd=DetailsSearch)]

The synthesis of [^111^In]-mAb806 (as a ^111^In-labeled [(R)-2-amino-3-(4-isothiocyanatophenyl)propyl]-trans(S,S)-cyclohexane-1,2-diethylenetriamine pentaacetic acid (CHX-A''-DTPA) conjugate of mAb806; [^111^In]-CHX-A”-DTPA-mAb806 or [^111^In]-mAb806) is described by Perera et al. (8). The radiochemical purity of the ^111^In-labeled mAb was reported to be 99.5% as determined with instant thin-layer chromatography, with a specific activity of 27 kBq/6.6 pmol (110.6 Ci/mmol). The final formulation and storage conditions of the labeled mAb were not reported.

For use as a control, another isotype-matched mAb, 100-310 (directed against the human A33 antigen), was labeled with ^111^In in a similar manner (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20in%20vitro&cmd=DetailsSearch)]

The immunoreactivity of [^111^In]-mAb806 was determined using A431 cells (a human epidermoid carcinoma cell line that expresses the EGFRvIII receptor) (8). The number of labeled mAb molecules bound per cell was reported to be 3.89 × 10^5^, which is similar to the number determined for the [^125^I]-labeled mAb806 (3.14 × 10^5^) (8). The isotype-matched ^111^In-labeled mAb 100-310 did not bind to the A431 cells under the same study conditions.

In another study, the internalization and trafficking of a fluorescent dye (Cy-3)–tagged mAb806 (mAb806-Cy3) was investigated using A431 cells (8). This study revealed that mAb806-Cy3 was internalized by the cells through a dynamin-dependent, clathrin-mediated, endocytotic process. The mAb was initially localized in the endosomes and later trafficked to and accumulated in the lysosomes (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=124I-IMP-R4-ch806%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-mAb806 was studied in BALB/c nude mice bearing xenograft A431 cell tumors (8). The animals were injected with the labeled mAb through the tail vein, and the mice were euthanized at predetermined time points (n = 4 animals/time point) for the collection of all major organs, including the tumors (6). In general, the uptake of label from [^111^In]-mAb806 by the tumors was higher than that from the [^125^I]-mAb806 at all time points (8). With [^111^In]-mAb806, the accumulation of radioactivity in the tumors increased from 21.8 ± 6.1 percent injected dose per gram tissue (% ID/g) at 4 h post-injection (p.i.) to 44.9 ± 11.4% ID/g at 48 h and reduced to 23.6 ± 6.3% ID/g by 168 h p.i. During the same time period, radioactivity in the blood from [^111^In]-mAb806 was observed to reduce from 30.9 ± 1.9% ID/g at 4 h p.i. to 12.6 ± 1.7% ID/g at 48 h p.i., and to further reduce to 5.2 ± 1.7 at 168 h p.i. To compare the accumulation of radioactivity from [^125^I]-mAb806 and [^111^In]-mAb806, respectively, in the tumors and the blood of the animals, the reader is referred to Table 1 in Perera et al. (8). All major organs were reported to have an accumulation of <10% ID/g radioactivity from [^111^In]-mAb806 at all time points. No blocking studies using unlabeled mAb806 or another suitable anti-EGFR mAb were reported.

On the basis of results obtained from these studies, the investigators concluded that [^111^In]-mAb806 could be an ideal candidate for development as a cancer detection or therapeutic agent (8).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-mAb%20806%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Spector N.L., Blackwell K.L. (2009). Understanding the mechanisms behind trastuzumab therapy for human epidermal growth factor receptor 2-positive breast cancer. J Clin Oncol.
2 Pines G., Kostler W.J., Yarden Y. (2010). Oncogenic mutant forms of EGFR: lessons in signal transduction and targets for cancer therapy. FEBS Lett.
3 Hasselbalch, B., U. Lassen, H.S. Poulsen, and M.T. Stockhausen, Cetuximab Insufficiently Inhibits Glioma Cell Growth Due to Persistent EGFR Downstream Signaling. Cancer Invest. 2010
4 Scott A.M., Lee F.T., Tebbutt N., Herbertson R., Gill S.S., Liu Z., Skrinos E., Murone C., Saunder T.H., Chappell B., Papenfuss A.T., Poon A.M., Hopkins W., Smyth F.E., MacGregor D., Cher L.M., Jungbluth A.A., Ritter G., Brechbiel M.W., Murphy R., Burgess A.W., Hoffman E.W., Johns T.G., Old L.J. (2007). A phase I clinical trial with monoclonal antibody ch806 targeting transitional state and mutant epidermal growth factor receptors. Proc Natl Acad Sci U S A.
5 Gan H.K., Kaye A.H., Luwor R.B. (2009). The EGFRvIII variant in glioblastoma multiforme. J Clin Neurosci.
6 Lee F.T., O'Keefe G.J., Gan H.K., Mountain A.J., Jones G.R., Saunder T.H., Sagona J., Rigopoulos A., Smyth F.E., Johns T.G., Govindan S.V., Goldenberg D.M., Old L.J., Scott A.M. (2010). Immuno-PET quantitation of de2-7 epidermal growth factor receptor expression in glioma using 124I-IMP-R4-labeled antibody ch806. J Nucl Med.
7 Jungbluth A.A., Stockert E., Huang H.J., Collins V.P., Coplan K., Iversen K., Kolb D., Johns T.J., Scott A.M., Gullick W.J., Ritter G., Cohen L., Scanlan M.J., Cavenee W.K., Old L.J. (2003). A monoclonal antibody recognizing human cancers with amplification/overexpression of the human epidermal growth factor receptor. Proc Natl Acad Sci U S A.
8 Perera R.M., Zoncu R., Johns T.G., Pypaert M., Lee F.T., Mellman I., Old L.J., Toomre D.K., Scott A.M. (2007). Internalization, intracellular trafficking, and biodistribution of monoclonal antibody 806: a novel anti-epidermal growth factor receptor antibody. Neoplasia.
9 Chopra, A., [111In]-Labeled CHX-A"-DTPA conjugated chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., [125I]-Labeled chimeric antibody 806 (ch806) targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
11 Chopra, A., [124I]-Labeled residulizing ligand IMP-R4 conjugated chimeric monoclonal antibody ch806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
12 Chopra, A., [125I]-Labeled monoclonal antibody 806 targeting the epidermal growth factor receptor deletion variant de2-7 (EGFRvIII). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.